# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-Tris-acetic acid-10-maleimidoethylacetamide-ACEQNPIYWARYADWLFTTPLLLLDLALLVDADEGTG

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-Tris-acetic acid-10-maleimidoethylacetamide-ACEQNPIYWARYADWLFTTPLLLLDLALLVDADEGTG
Abbreviated name: | ^64^Cu-DOTA-pHLIP
Synonym:
Agent Category: | Peptide
Target: | Low extracellular pH (pH_e_)
Target Category: | Other
Method of detection: | Position emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP)]

The pH low insertion peptide (pHLIP) is a peptide of 37 amino acids that inserts across the cell membrane as an α-helix when the extracellular pH (pH_e_) is acidic (1-3). pHLIP labeled with ^64^Cu (^64^Cu-DOTA-pHLIP) was developed by Vāvere et al. as a positron emission tomography (PET) tracer for delineation of the low pH_e_ in tumors (3). The half-life of ^64^Cu is 12.74 hours.

Tumor microenvironment is characterized by low pH_e_ (4, 5). Almost all solid tumors have a neutral to alkaline intracellular pH (pH_i_), but they develop an acidic pH_e_ (known as the Warburg effect, Nobel Prize in 1931 (http://nobelprize.org/nobel_prizes/medicine/laureates/1931)). The average pH_e_ could be as low as 6.0 (6-8). A pH gradient (pH_i_ > pH_e_) exists across the cell membrane in tumors. This gradient is contrary to that found in normal tissues, in which pH_i_ is lower than pH_e_ (7.2–7.4) (6-8). Diffusion of the H^+^ ions along concentration gradients from tumors into adjacent normal tissues creates a peritumoral acid gradient (9). The mechanisms responsible for the low pH_e_ include anaerobic glycolysis because of hypoxia, aerobic glycolysis (the Warburg effect), increased metabolic CO_2_ production associated with uncontrolled cell growth, and increased activity of ion pumps on the cell membrane (4, 6).

Low pH_e_ affects many aspects of tumor physiology. It is one of the driving forces in the clonal selection leading to invasive and metastatic diseases (10, 11). Rofstad et al. have shown that lowering culture pH to 6.8 results in a promotion of in vivo metastasis of treated tumor cells compared with controls (cultured at pH 7.4) after tail vein injection in mice (12). Exposure of tumor cells to an acidic environment leads to increased expression of various factors that contribute to tumor progression (11). Tumor cells are able to maintain a high proliferation rate in the acidic environment, whereas the peritumoral acid gradient limits immune response to tumor antigens and induces normal cell apoptosis, extracellular matrix degradation, and angiogenesis (6, 10). The passage of noncarrier-mediated weak drugs through the cell membranes is also influenced by the acidic pH_e_ (13-15). Typically, the drugs in an uncharged state (lipophilic form) pass more efficiently through the cell membranes. This leads to the hypothesis of ‘ion-trapping’ that weakly basic drugs will concentrate in more acidic compartments (13, 14). The acid pH_e_ of tumors will therefore hinder weakly basic drugs from reaching their intracellular targets, thereby reducing cytotoxicity (15). Conversely, the acid pH_e_ of tumors will improve uptake of weak acids into the relatively neutral intracellular space (16). The currently used chemotherapeutic drugs such as mitoxantrone, doxorubicin, daunorubicin, anthracyclines, anthraquinones and vinca alkaloids are all weak bases (pKa 5.5–6.8), while cyclophosphamide, 5-fluorouracil and chlorambucil are weak acids (pKa 7.8–8.8) (14). Both in vitro and in vivo studies have shown that the activities of those weak bases are inhibited by the low pH_e_ (13-15). On the contrary, the actions of the weak acids are enhanced by the low pH_e_. The pH gradient in tumors exerts a protective effect upon the cells from weak-base drugs as well as acts to potentiate the action of weak acid drugs (16). Studies have consistently shown that selective tumor alkalinization in vivo is likely to result in an enhancement in the anti-tumor activity of weakly basic chemotherapeutic drugs (17, 18). Low pH_e_ has also been shown to impair the effectiveness of some drugs such as paclitaxel in that their chemical structures do not predict pH-dependent ionization (6). In addition, radiation therapies are known to be significantly less effective at the hypoxic and acidic regions of tumor (19).

An understanding of the mechanisms involved in tumor-specific low pH_e_ leads to the development of targeted therapeutic approaches (5, 6). Low pH_e_ is also considered a promising marker for tumor targeting detection (3, 7). Vāvere et al. have synthesized and described the use of ^64^Cu-DOTA-pHLIP for delineation of low pH_e_ in prostate tumors (3). The pHLIP interacts with the surface of membranes as an unstructured peptide at neutral pH_e_, but at acidic pH_e_ (<7.0) it inserts across the membrane and forms a stable transmembrane α-helix (1, 20-22). The pHLIP affinity for membranes at low pH (5.0) is 20 times higher than that at high pH (8.0). Studies by Zoonens et al. showed that the pHLIP could translocate cell-impermeable cargo molecules across a cell membrane and release them in the cytoplasm (23). The process is mediated by the formation of a transmembrane α-helix because of increased peptide hydrophobicity associated with the protonation of Asp residues at low pH (21, 22). Replacement of the two key Asp residues located in the transmembrane part of pHLIP with Lys or Asn leads to the loss of pH-sensitive membrane insertion (2). With in vivo PET imaging, Vāvere et al. have shown that ^64^Cu-DOTA-pHLIP delineates low pH_e_ in prostate tumor xenografts (3).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP+pH+imaging)]

The synthesis of ^64^Cu-DOTA-pHLIP and ^64^Cu-DOTA-K-pHLIP was described in detail by Vāvere et al. (3). The sequence of pHLIP is ACEQNPIYWARYADWLFTTPLLLLDLALLVDADEGTG. K-pHLIP is a mutant version of pHLIP in which the key Asp residues of the transmembrane part of pHLIP are replaced by positively charged Lys residues (ACEQNPIYWARYAKWLFTTPLLLLKLALLVDADEGTG). Because of the replacement, K-pHLIP has lost its pH-sensitive nature, and it is used as a control in the study. Both peptides were prepared with solid-phase peptide synthesis and purified with reverse-phase chromatography. The NH_2_ terminus of the peptides was first covalently conjugated to 1,4,7,10-tetraazacyclododecane-1,4,7-Tris-acetic acid-10-maleimidoethylacetamide, a maleimide-containing derivative of DOTA. The conjugates were then radiolabeled by incubation with ^64^Cu at a ratio of 1:1 (µg:mCi) in 0.5 mol/L ammonium acetate (pH 5.5) for 30 min at 25°C. After purification, the labeled solutions were reported to be stable overnight without heating. The specific activity of ^64^Cu-DOTA-pHLIP and ^64^Cu-DOTA-K-pHLIP was 58.8 and 63.4 GBq/µmol (1,591 and 1,713 mCi/µmol), respectively. The radiochemical purity was >95% for both conjugates.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP+pH+imaging)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP+pH+imaging)]

Vāvere et al. analyzed the acute biodistribution of ^64^Cu-DOTA-pHLIP in PC-3 and LNCaP xenograft-bearing mice (3). The tumor xenografts were implanted in the right flank of male athymic mice. ^64^Cu-DOTA-pHLIP (~1.04 GBq (28 µCi)) was injected intravenously to mice with tumors that were 0.5–0.75 cm^3^ in volume. An additional group of PC-3–bearing mice (n = 5) received an equivalent mass of ^64^Cu-DOTA-K-pHLIP as a control. Animals were euthanized at different time points after injection (1, 4, 24, and 48 h; n = 4–5 mice). To investigate the tumor accumulation of ^64^Cu-DOTA-pHLIP after modulation of the tumor pH, a cohort of LNCaP-bearing mice (n = 8) was split into two groups, with the first group receiving 150 mmol/L bicarbonated water (pH 8.0) ad libitum for 7 days (modulated group), and the second group receiving regular drinking water (nonmodulated group). Analysis showed that there was no significant difference between PC-3 and LNCaP tumor models for the ^64^Cu-DOTA-pHLIP distribution in the blood and blood-rich organs such as liver, lung, heart, and spleen. In the PC-3 tumors, ^64^Cu-DOTA-pHLIP accumulation reached the maximum (2.78 ± 0.19% injected dose per gram (ID/g)) after 4 h. In the LNCaP tumors, ^64^Cu-DOTA-pHLIP accumulation reached the maximum (4.50 ± 1.71% ID/g) after 1 h and was still high with 3.23 ± 0.55% ID/g at 24 h and 1.74 ± 1.41% ID/g at 48 h after injection, respectively. The distribution of the control, ^64^Cu-DOTA-K-pHLIP, exhibited a pattern similar to that of the ^64^Cu-DOTA-pHLIP, although accumulation was lower in all tissues. However, the amount of ^64^Cu-DOTA-K-pHLIP was ~40% less than that of ^64^Cu-DOTA-pHLIP in the PC-3 tumors at 1 h after injection. As the ^64^Cu-DOTA-pHLIP was given to the LNCaP-bearing mice with or without modulation, no difference was observed between the two groups for its accumulation in the 17 collected organs except for the tumor and kidney. The uptake of ^64^Cu-DOTA-pHLIP was significantly higher (P = 0.005) in the nonmodulated tumors than in the modulated tumors (4.50 ± 1.71 versus 1.31 ± 0.60% ID/g, respectively). In the kidney, ^64^Cu-DOTA-pHLIP uptake was 5.20 ± 1.06 and 3.78 ± 0.29% ID/g (P < 0.005) in the nonmodulated and modulated mice, respectively.

Vāvere et al. performed small-animal PET imaging with ^64^Cu-DOTA-pHLIP on the two tumor models (PC-3, n = 4 mice; LNCaP, n = 10 mice) (3). ^64^Cu-DOTA-pHLIP (7.4 MBq (200 µCi)) was injected via tail vein. Images were evaluated by analyzing the standardized uptake value (SUV) of the tumors and muscles. In the PC-3 model, the tumor/muscle ratios derived from the SUVs at 1, 4, and 24 h were 1.45 ± 0.09, 2.67 ± 0.40, and 4.64 ± 1.08, respectively, showing a gradual increase in tumor uptake with concurrent washout from nontarget organs. The tumor/muscle ratios in the LNCaP tumors were significantly higher (P = 0.0001) than in the PC-3 tumors, with values of 3.44 ± 0.50, 5.56 ± 0.21, and 6.55 ± 1.98 for the 1, 4, and 24 h time points, respectively. ^64^Cu-DOTA-K-pHLIP did not exhibit any targeting ability (data not shown by the authors).

The differences in the ^64^Cu-DOTA-pHLIP PET imaging between LNCaP and PC-3 tumors, and between modulated and nonmodulated LNCaP tumors, were mirrored in the pH values determined with magnetic resonance spectroscopy (MRS). Based on the ^31^P magnetic resonance-observable chemical shift of 3-aminopropylphosphonate (3-APP), MRS showed that the LNCaP tumors had a more acidic average pH_e_ (6.78 ± 0.29) than the PC-3 tumors (7.23 ± 0.10) (P = 0.039). The average pH_e_ was also more acidic in the nonmodulated LNCaP tumors than in the modulated LNCaP tumors (6.62 ± 0.35 versus 6.94 ± 0.56, respectively), although the pH_e_ difference did not reach statistical significance (P = 0.28) (3). However, MRS measures the volume-average pH_e_ of tumors and is not a direct measure of the pH that causes pHLIP insertion. Vāvere et al. concluded that ^64^Cu-DOTA-pHLIP offers the possibility of designing a new class of noninvasive pH-selective PET imaging agents that will be useful for the imaging of a broad range of disease states (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP+pH+imaging)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP+pH+imaging)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=pHLIP+pH+imaging)]

No references are currently available.

## References

1 Reshetnyak Y.K., Andreev O.A., Lehnert U., Engelman D.M. (2006). Translocation of molecules into cells by pH-dependent insertion of a transmembrane helix. Proc Natl Acad Sci U S A.
2 Reshetnyak Y.K., Segala M., Andreev O.A., Engelman D.M. (2007). A monomeric membrane peptide that lives in three worlds: in solution, attached to, and inserted across lipid bilayers. Biophys J.
3 Vavere A.L., Biddlecombe G.B., Spees W.M., Garbow J.R., Wijesinghe D., Andreev O.A., Engelman D.M., Reshetnyak Y.K., Lewis J.S. (2009). A novel technology for the imaging of acidic prostate tumors by positron emission tomography. Cancer Res.
4 Fukumura D., Jain R.K. (2007). Tumor microenvironment abnormalities: causes, consequences, and strategies to normalize. J Cell Biochem.
5 Izumi H., Torigoe T., Ishiguchi H., Uramoto H., Yoshida Y., Tanabe M., Ise T., Murakami T., Yoshida T., Nomoto M., Kohno K. (2003). Cellular pH regulators: potentially promising molecular targets for cancer chemotherapy. Cancer Treat Rev.
6 Cairns R., Papandreou I., Denko N. (2006). Overcoming physiologic barriers to cancer treatment by molecularly targeting the tumor microenvironment. Mol Cancer Res.
7 Pathak A.P., Gimi B., Glunde K., Ackerstaff E., Artemov D., Bhujwalla Z.M. (2004). Molecular and functional imaging of cancer: advances in MRI and MRS. Methods Enzymol.
8 Penet M.F., Glunde K., Jacobs M.A., Pathak A.P., Bhujwalla Z.M. (2008). Molecular and functional MRI of the tumor microenvironment. J Nucl Med.
9 Gatenby R.A., Gawlinski E.T., Gmitro A.F., Kaylor B., Gillies R.J. (2006). Acid-mediated tumor invasion: a multidisciplinary study. Cancer Res.
10 Lunt S.J., Chaudary N., Hill R.P. (2009). The tumor microenvironment and metastatic disease. Clin Exp Metastasis.
11 Joyce J.A., Pollard J.W. (2009). Microenvironmental regulation of metastasis. Nat Rev Cancer.
12 Rofstad E.K., Mathiesen B., Kindem K., Galappathi K. (2006). Acidic extracellular pH promotes experimental metastasis of human melanoma cells in athymic nude mice. Cancer Res.
13 Raghunand N., Mahoney B.P., Gillies R.J. (2003). Tumor acidity, ion trapping and chemotherapeutics. II. pH-dependent partition coefficients predict importance of ion trapping on pharmacokinetics of weakly basic chemotherapeutic agents. Biochem Pharmacol.
14 Mahoney B.P., Raghunand N., Baggett B., Gillies R.J. (2003). Tumor acidity, ion trapping and chemotherapeutics. I. Acid pH affects the distribution of chemotherapeutic agents in vitro. Biochem Pharmacol.
15 Gerweck L.E., Kozin S.V., Stocks S.J. (1999). The pH partition theory predicts the accumulation and toxicity of doxorubicin in normal and low-pH-adapted cells. Br J Cancer.
16 Kozin S.V., Shkarin P., Gerweck L.E. (2001). The cell transmembrane pH gradient in tumors enhances cytotoxicity of specific weak acid chemotherapeutics. Cancer Res.
17 Silva A.S., Yunes J.A., Gillies R.J., Gatenby R.A. (2009). The potential role of systemic buffers in reducing intratumoral extracellular pH and acid-mediated invasion. Cancer Res.
18 Swietach P., Vaughan-Jones R.D., Harris A.L. (2007). Regulation of tumor pH and the role of carbonic anhydrase 9. Cancer Metastasis Rev.
19 Vaupel P. (2004). Tumor microenvironmental physiology and its implications for radiation oncology. Semin Radiat Oncol.
20 Tang J., Gai F. (2008). Dissecting the membrane binding and insertion kinetics of a pHLIP peptide. Biochemistry.
21 Reshetnyak Y.K., Andreev O.A., Segala M., Markin V.S., Engelman D.M. (2008). Energetics of peptide (pHLIP) binding to and folding across a lipid bilayer membrane. Proc Natl Acad Sci U S A.
22 Andreev O.A., Dupuy A.D., Segala M., Sandugu S., Serra D.A., Chichester C.O., Engelman D.M., Reshetnyak Y.K. (2007). Mechanism and uses of a membrane peptide that targets tumors and other acidic tissues in vivo. Proc Natl Acad Sci U S A.
23 Zoonens M., Reshetnyak Y.K., Engelman D.M. (2008). Bilayer interactions of pHLIP, a peptide that can deliver drugs and target tumors. Biophys J.